# 2-[methyl-^11^C]Methoxyestradiol

Chemical name: | 2-[methyl-^11^C]Methoxyestradiol
Abbreviated name: | [^11^C]2-ME
Synonym:
Agent Category: | Compound
Target: | Superoxide dismutase
Target Category: | Enzyme binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=2-methoxyestradiol)]

Endothelial cells are important cells in angiogenesis (1). Tumor growth requires the formation of new blood vessels. Potent angiogenic factors (e.g., vascular endothelial growth factor and basic fibroblast growth factor) induce proliferation, sprouting, migration, and tube formation of endothelial cells (2). 2-Methoxyestradiol (2-ME), an endogenous metabolite of 17β-estradiol, inhibits proliferating tumor cells and angiogenesis in vitro and in vivo (3, 4). It also inhibits the proliferation of endothelial cells and has low affinity for estrogen receptors. Huang et al. (5) demonstrated that the anti-proliferation effect of 2-ME may be the result of its inhibition of superoxide dismutase (SOD) and induction of apoptosis. Inhibition of SOD leads to free radical–mediated damage to mitochondrial membranes resulting in apoptosis. 2-[methyl-^11^C]Methoxyestradiol ([^11^C]2-ME) has been evaluated as an imaging probe to study angiogenesis (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-methoxyestradiol%20and%20synthesis)]

[^11^C]2-ME was synthesized from its precursor, 2-hydroxy-3,17β-estradiol-3,17-bis(methoxymethyl)ether, by O-methylation by use of ^11^C-methyl iodide (NaH, 80°C for 6 min), followed by acid hydrolysis (HCl, 80°C for 6 min) (6). [^11^C]2-ME was purified by reverse-phase high-performance liquid chromatography. The radiochemical yields (decay-corrected) on the basis of [^11^C]CH_3_I were 25–34%, and the specific activities were 34–38 GBq/µmol (0.92–1.03 Ci/µmol) at the end of synthesis. The total synthesis time was 60–65 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-methoxyestradiol%20and%20in%20vitro)]

Fotsis et al. (3) reported that 2-ME (10 μM) inhibited proliferation of human umbilical vein endothelial cells (HUVECs) by >85%. Lee et al. (6) showed that [^11^C]2-ME accumulated in HUVECs with 2.96% injected dose (ID) at 5 min, 4.74% ID at 15 min, 6.51% ID at 30 min, and 7.10% ID at 60 min. 2-ME (10 μM) inhibited the uptake at 60 min by 70%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-methoxyestradiol%20and%20rodentia)]

Lee et al. (6) performed biodistribution studies of [^11^C]2-ME in mice bearing a Lewis lung carcinoma tumor in the right flank. The organs with the highest accumulation of [^11^C]2-ME (% ID/g) were the liver (9.34 ± 2.12), lung (3.36 ± 0.09), and kidneys (3.26 ± 0.55) at 60 min after injection. The tumor (1.04 ± 0.27% ID/g) exhibited a tumor/muscle ratio of 2.36, which would provide a good contrast for tumor imaging. No blocking experiment was performed. In normal mice, [^11^C]2-ME showed a distribution half-life (t_1/2_α) and an elimination half-life (t_1/2_β) of 0.36 and 19 min, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-methoxyestradiol%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-methoxyestradiol%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=2-methoxyestradiol%20and%20human)]

No publication is currently available.

## References

1 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
2 Distler J.H., Hirth A., Kurowska-Stolarska M., Gay R.E., Gay S., Distler O. (2003). Angiogenic and angiostatic factors in the molecular control of angiogenesis. Q J Nucl Med.
3 Fotsis T., Zhang Y., Pepper M.S., Adlercreutz H., Montesano R., Nawroth P.P., Schweigerer L. (1994). The endogenous oestrogen metabolite 2-methoxyoestradiol inhibits angiogenesis and suppresses tumour growth. Nature.
4 Klauber N., Parangi S., Flynn E., Hamel E., D'Amato R.J. (1997). Inhibition of angiogenesis and breast cancer in mice by the microtubule inhibitors 2-methoxyestradiol and taxol. Cancer Res.
5 Huang P., Feng L., Oldham E.A., Keating M.J., Plunkett W. (2000). Superoxide dismutase as a target for the selective killing of cancer cells. Nature.
6 Lee I., Seong Choe Y., Jung K.H., Lee K.H., Young Choi J., Choi Y., Kim B.T. (2007). 2-[methyl-(11)C]Methoxyestradiol: synthesis, evaluation and pharmacokinetics for in vivo studies on angiogenesis. Nucl Med Biol.